# [^125^I](E)-N-1-(3'-iodoallyl)-N'-4-(3'',4''-dimethoxyphenethyl)-piperazine

Chemical name: | [^125^I](E)-N-1-(3'-iodoallyl)-N'-4-(3'',4''-dimethoxyphenethyl)-piperazine | [image]
Abbreviated name: | [^125^I]E-1 | [image]
Synonym: | | [image]
Agent Category: | Compounds | [image]
Target: | Sigma-1 (σ1) receptor | [image]
Target Category: | Receptors | [image]
Method of detection: | Single-photon emission computed tomography (SPECT) | [image]
Source of signal / contrast: | ^125^I | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structures of E-1, Z-1, 2, and 3 (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=sigma-1%20receptors%20and%20imaging)]

[^125^I](E)-N-1-(3'-iodoallyl)-N'-4-(3'',4''-dimethoxyphenethyl)-piperazine, abbreviated as [^125^I]E-1, is a hybrid structure of two known ligands: TPCNE (1(trans-iodopropen-2-yl)-4-[(4-cyanophenoxy)methyl]piperidine) and SA4503 (1-[2-(3,4-dimethoxyphenethyl)]-4-(3-phenylpropyl)piperazine). [^125^I]E-1 was synthesized for use with single-photon emission computed tomography (SPECT) of sigma-1 (σ1) receptors (1).

σ1 receptor is a protein that is widely distributed in both the central nervous system (CNS) and peripheral organs. There are at least two subtypes of σ receptors, σ1 receptor and σ2 receptor. Although the functions of σ2 receptor are poorly understood, σ1 receptor is believed to act as a modulator of the signal transduction in neurotransmitter systems (2, 3). σ1 receptor primarily resides at the interface between the endoplasmic reticulum and mitochondria, where it modulates Ca^2+^ flux by acting as a molecular chaperone for type 3 inositol-1,4,5-triphosphate receptors. σ1 receptor can also translocate to the plasma membrane, where it regulates the voltage-dependent Ca^2+^ channels, K^+^ channels, and other membrane-bound proteins (2, 4).

Increasing evidence suggests that σ1 receptor is involved in a range of CNS diseases such as affective disorders, psychosis, schizophrenia, substance abuse, Parkinson’s disease, and Alzheimer’s disease (4, 5). Studies on postmortem human brains have shown that the density of σ1 receptor decreased in patients with schizophrenia and Alzheimer’s disease (6). Discovery of specific ligands for σ1 receptors has further prompted development of efficient imaging probes for neuropsychiatric diseases by targeting σ1 receptor (3, 5).

TPCNE and SA4503 are among the radiotracers investigated for σ receptor imaging. TPCNE has an affinity of K_i_ = 0.67 nM (log P = 3.36) for σ1 receptors, and SA4503 has an affinity of K_i_ = ~5 nM (log P = 2.52) for σ1 receptors (7-9). Both exhibit good specific binding to σ1 receptors in rat brains and in human brains. Lever et al. synthesized four hybrid structure–related N-1-allyl-N'-4-phenethylpiperazines (E-1, Z-1, 2, and 3) from TPCNE and SA4503 on the basis of the hypothesis that hybrid structures might be suitable scaffolds for developing radioiodinated ligands that have high σ1 receptor affinities and appropriate lipophilicities for in vivo studies (1). Lever et al. selected E-1 and Z-1 to probe the effect of geometric isomerism upon σ receptor binding and to discriminate the contribution of the iodine atom through comparison with the allyl analog 2 (1). Compound 3, which is a monomethyl analog and is likely to be a metabolite of E-1, was used in the studies to determine the radiometabolites of [^125^I]E-1. The results obtained by Lever et al. showed that [^125^I]E-1 was a selective σ1 receptor antagonist that exhibited properties amenable to in vitro and in vivo studies, with possible extension to SPECT using iodine-123 (1).

### Related Resource Links:

The nucleotide (http://www.ncbi.nlm.nih.gov/nuccore?term=sigma-1%20receptors) and protein (http://www.ncbi.nlm.nih.gov/protein?term=sigma-1%20receptors) sequences of sigma-1 (σ1) receptors

Sigma-1 (σ1) receptor-related compounds (http://www.ncbi.nlm.nih.gov/pcsubstance?term=sigma-1%20receptors) in PubChem

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=22172395)]

Lever et al. described the synthesis of E-1, Z-1, 2, and 3 in detail (1). E-1 and Z-1 were prepared with comparable overall yields (E-1, 31%; Z-1, 36%) over four-step synthesis. Synthesis of the allyl analog 2 was accomplished by alkylation of commercially available N-allylpiperazine in one step, with an unoptimized yield of 29%. The synthesis of compound 3 was achieved through multiple steps, with a yield of 70% for the final step. The full chemical names of E-1, Z-1, 2, and 3 are (E)-N-1-(3'-iodoallyl)-N'-4-(3'',4''-dimethoxyphenethyl)-piperazine, (Z)-N-1-(3'-iodoallyl)-N'-4-(3'',4''-dimethoxyphenethyl)-piperazine, N-1-allyl-N'-4-(3',4'-dimethoxyphenethyl)-piperazine, and (E)-N-1-(3'-iodoallyl)-N'-4-(3''-methoxy-4''-hydroxyphenethyl)-piperazine, respectively.

[^125^I]E-1 and [^125^I]Z-1 were prepared from their corresponding stannyl precursors, with radiochemical yields of 74%–82%, radiochemical purities of >98%, and specific radioactivities of 71.6–77.3 GBq/µmol (1.94–2.09 Ci/μmol) (1). Incorporation of radioactivity was ~90%. Both [^125^I]E-1 and [^125^I]Z-1 showed >95% radiochemical purity after 2 weeks of storage at −20°C in the dark in EtOH, and the agents maintained 95% purity after 30 days.

The lipophilicity (log D_7.4_) of [^125^I]E-1 and [^125^I]Z-1 was determined by partitioning 74–148 kBq (2–4 μCi) of each agent between equal volumes of n-octanol and Dulbecco's phosphate-buffered saline (0.1 M, pH 7.4) (n = 5) (1). The results showed that the log D_7.4_ values (means ± SD) of [^125^I]E-1 (2.25 ± 0.008) and [^125^I]Z-1 (2.27 ± 0.006) were in the optimal range for in vivo utility and were similar to the log P value of SA4503 (2.52), but lower than the log P value of TPCNE (3.36) (7, 9). The calculated lipophilicities of compounds 2 (1.77) and 3 (2.06) were lower than those of [^125^I]E-1 and [^125^I]Z-1.

The protein binding of [^125^I]E-1 was assessed with the trichloroacetic acid method after incubation with mouse plasma for 30 min at 37°C (1). [^125^I]E-1 showed a modest binding with plasma proteins (48.2 ± 1.0%, n = 4). The protein binding was not assessed for other compounds.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=22172395)]

The binding and selectivity of E-1, Z-1, 2, and 3 for σ receptors in guinea pig brain were measured with competition binding assays using [^3^H](+)-pentazocine (σ_1_) and [^3^H]ditolylguanidine ([^3^H]DTG) (σ_2_) as radioligands (1).

Binding assays with guinea pig brain homogenates revealed significant differences in binding affinity and σ_1_/σ_2_ selectivity for the four compounds (Table 1). E-1, Z-1, and 3, which contained the N-iodoallyl moiety, displayed similar, moderately high σ_1_ receptor affinities. By contrast, compound 2, which contained the N-allyl group, showed a σ_1_ receptor affinity one order of magnitude lower. These results indicated that the σ_1_ receptor affinity was not sensitive to the E and Z geometric isomerism, but iodine contributed to the binding at σ_1_ sites. For σ_2_ receptor binding, the sensitivity was high to the structure, where a 300-fold range was observed for the four analogs. Compound 3 displayed the highest affinity; E-1 and Z-1 exhibited relatively poor affinity, and compound 2 exhibited the poorest affinity with a K_i_ > 10 μM. These results indicated that a free phenol led to a much stronger σ_2_ binding interaction than a methoxy group. Overall, E-1 had the highest affinity and best selectivity for σ_1_ receptor binding. Compared with SA4503 and TPCNE, E-1 exhibited greater selectivity for binding to σ_1_ sites over σ_2_ sites, accompanied by a 3- to 20-fold weaker apparent σ_1_ binding affinity.

Table 1. In vitro binding properties for σ receptors.

Compound | σ1 (K_i_ = nM) | σ2 (K_i_ = nM) | σ1/σ2 ratio
E-1 | 15.1 ± 1.3 | 1,263 ± 166 | 84
Z-1 | 19.9 ± 1.3 | 455 ± 66 | 23
2 | 132 ± 12 | 10,950 ± 1,295 | 83
3 | 13.0 ± 0.5 | 36.6 ± 1.0 | 3
SA4503 | 4.6 ± 0.2^a^ | 63.1 ± 4.3^a^ | 14
TPCNE | 0.67^b^ | 38.8^b^ | 58

Values are means ± SEM (n = 3–4) from competition assays against [^3^H](+)-pentazocine (σ1) and [^3^H]DTG (σ2) in membrane homogenates from male guinea pig brains.

^a^Data from Lever et al. (8).

^b^Data from Waterhouse et al. (10).

Compound E-1 was further checked for its binding to other receptors against a panel of six well-characterized radioligands in brain membrane homogenates (data not shown). Low displacements were noted for κ (6%), δ (6%), and μ (34%) opioid receptors, as well as dopamine (8%), norepinephrine (2%), and serotonin transporters (35%). Thus, K_i_ values for E-1 against opioid receptors and monoamine transporters were likely >10 μM.

A σ1 competition assay was also conducted in the presence of phenytoin. Phenytoin is an allosteric modulator of the σ_1_ receptor binding that induces a shift to higher affinity for a number of known agonists, but a slight shift to lower affinity for many antagonists (11). The competition assay showed that the half maximal inhibitory concentration for E-1 exhibited a modest but significantly different shift to lower affinity (30.4 ± 2.6 nM; Hill slope 1.03 ± 0.06) in the presence of phenytoin as compared to the NaOH vehicle control (21.1 ± 0.06 nM; Hill slope 1.03 ± 0.04) (P = 0.02). These findings are consistent with designation of E-1 as a putative antagonist.

To define the nonspecific binding of [^125^I]E-1 in vitro, Lever et al. conducted a series of assays using membrane homogenates from whole CD1 mouse brains (1). Association studies indicated that the pseudoequilibrium was reached within 60 min, and ≥95% specific binding was observed over the plateau from 60 min to 240 min. Specific binding of [^125^I]E-1 increased linearly (r^2^ = 1.0) over a protein range of 100–400 mg (data not shown). Homologous competition studies with a 60-min incubation time and 0.2 mg protein showed saturable binding for [^125^I]E-1 that fitted a one-site model (r^2^ = 1.0). The K_d_ was 3.79 ± 0.21 nM, and the B_max_ was 599 ± 28 fmol/mg protein.

Inhibitory potency studies for several σ receptor ligands in competition against [^125^I]E-1 showed a rank order of potency: haloperidol > (+)-pentazocine > BD1063 >> DTG (1). These data supported the selective, saturable binding of [^125^I]E-1 to σ_1_ receptor sites in mouse brain membrane homogenates, with highly specific binding and moderately high binding affinity.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=22172395)]

The pharmacokinetics of [^125^I]E-1 and [^125^I]Z-1 were determined after intravenous administration of each radioligand (92.5 kBq; 2.5 μCi) to male CD1 mice (n = 4 mice/time point) (1). Within 15 min, there was a trend for [^125^I]E-1 to show higher organ uptake than [^125^I]Z-1. The blood level of [^125^I]E-1 was significantly lower than that of [^125^I]Z-1 (P = 0.01). The brain/blood ratio for [^125^I]E-1 at 15 min was 13.4, while that for [^125^I]Z-1 was 5.8. By 60 min, the levels of [^125^I]E-1 were significantly higher than those of [^125^I]Z-1 in all examined organs (P ≤ 0.006) except for pancreas, which maintained through 120 min.

[^125^I]E-1 and [^125^I]Z-1 readily crossed the blood–brain barrier. [^125^I]E-1 exhibited higher brain uptake and longer retention than [^125^I]Z-1. [^125^I]E-1 clearance from brain was monoexponential (r^2^ = 0.99; t_½_ = 36 min), with 5.8% injected dose per gram tissue (ID/g) peak uptake at 15 min, which decreased to 1.5% ID/g by 120 min. [^125^I]Z-1 was also cleared from brain as a first-order decline (r^2^ = 0.99; t_½_ = 16 min), from 4.8% ID/g at 15 min to 0.6% ID/g at 120 min. Washouts of both radioligands from heart, lung, and muscle also fit monoexponential curves (r^2^ ≥ 0.98) over 15–120 min. In these organs, the half-life values for [^125^I]E-1 were 1.5–2.5 times longer than those for [^125^I]Z-1 (data not shown).

Specific binding of [^125^I]E-1 and [^125^I]Z-1 was evaluated with various σ receptor ligands including haloperidol, BD1063 (σ1), Br-Mach (σ2), and nonradioactive E-1 and Z-1 compounds (1). Uptake of [^125^I]E-1 in most organs was saturable by pretreatment with nonradioactive E-1 and blocked by pretreatment with haloperidol (σ1/σ2) and the σ1 receptor-selective BD1063, but not by pretreatment with σ2 receptor-selective Br-Mach. As defined by BD1063, the specific binding of [^125^I]E-1 to σ1 receptors was 80% in brain, 44% in heart, 61% in lung, 68% in spleen, 65% in pancreas, and 57% in liver. Uptake of the [^125^I]E-1 in muscle (0.70% ID/g) was reduced significantly by BD1063 (48%) and E-1 (58%), but any changes with haloperidol or Br-Mach were not significant. Kidney uptake (3.71% ID/g) was not affected by pretreatment with any of these ligands (data not shown). Uptake of the [^125^I]Z-1 at 60 min was blocked significantly by haloperidol in all organs (P < 0.01) with the exception of heart (P = 0.08). Muscle uptake (0.46%ID/g) was also inhibited (19%; P = 0.02), but kidney uptake (3.42% ID/g) was not (P = 0.71) (data not shown). As defined by haloperidol, the specific binding of [^125^I]Z-1 was 74% in brain, 40% in lung, and 57%–65% across spleen, pancreas, and liver.

Radiometabolite studies were performed with brain and liver extracts, as well as serum and urine samples at 60 min after intravenous administration of [^125^I]E-1 (3.7 MBq; 100 μCi) to a male CD1 mouse (1). Radioactivity was extracted efficiently (98%) from brain tissue and consisted primarily of the unmetabolized [^125^I]E-1 (92%, t_R_ = 8.75 min). One minor (8%), less lipophilic metabolite was observed at 3.75 min with high-performance liquid chromatography (HPLC). By contrast, only 69% of the total radioactivity could be extracted from liver. Two minor metabolites, one at 3.75 min (3.5%) and the other at 1.75 min (6.5%), were noted along with unmetabolized [^125^I]E-1 (90%). Recovery of radioactivity from heart, lung, spleen, and pancreas was nearly complete (99%), and the proportion of unmetabolized [^125^I]E-1 ranged from 88% to 96% (data not shown). Low levels of the two minor metabolites observed in the liver extract were also observed to varying degrees in the other peripheral organs. Serum showed 12% unmetabolized [^125^I]E-1 along with 88% polar radiometabolites. Urine consisted almost exclusively of the polar radiometabolites. The data indicated that the polar radiometabolites in serum did not cross the blood–brain barrier.

Aryl methoxy groups are prone to O-demethylation in vivo by cytochrome P450 enzymes in liver and, to a lesser extent, brain. Therefore, the radiometabolite of [^125^I]E-1 having intermediate lipophilicity (t_R_ = 3.75 min) could be a simple phenol. Another possibility is that it was a des-methyl congener of [^125^I]E-1. The monomethyl analog 3 had the same retention time as this radiometabolite under the HPLC conditions (data not shown). Thus, the radiometabolite with t_R_ = 3.75 min observed in brain and peripheral organs was likely to be [^125^I]3 or the des-methyl congener of [^125^I]E-1.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=22172395)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=22172395)]

No references are currently available.

## References

1 Lever S.Z., Xu R., Fan K.H., Fergason-Cantrell E.A., Carmack T.L., Watkinson L.D., Lever J.R. (2012). Synthesis, radioiodination and in vitro and in vivo sigma receptor studies of N-1-allyl-N -4-phenethylpiperazine analogs. Nucl Med Biol.
2 Diaz J.L., Zamanillo D., Corbera J., Baeyens J.M., Maldonado R., Pericas M.A., Vela J.M., Torrens A. (2009). Selective sigma-1 (sigma1) receptor antagonists: emerging target for the treatment of neuropathic pain. Cent Nerv Syst Agents Med Chem.
3 Berardi F., Abate C., Ferorelli S., Colabufo N.A., Perrone R. (2009). 1-Cyclohexylpiperazine and 3,3-dimethylpiperidine derivatives as sigma-1 (sigma1) and sigma-2 (sigma2) receptor ligands: a review. Cent Nerv Syst Agents Med Chem.
4 Moussa I.A., Banister S.D., Giboureau N., Meikle S.R., Kassiou M. (2011). Synthesis and in vivo evaluation of [18F]N-(2-benzofuranylmethyl)-N'-[4-(2-fluoroethoxy)benzyl]piperazine, a novel sigma1 receptor PET imaging agent. Bioorg Med Chem Lett.
5 Moussa I.A., Banister S.D., Beinat C., Giboureau N., Reynolds A.J., Kassiou M. (2010). Design, synthesis, and structure-affinity relationships of regioisomeric N-benzyl alkyl ether piperazine derivatives as sigma-1 receptor ligands. J Med Chem.
6 Jansen K.L., Faull R.L., Storey P., Leslie R.A. (1993). Loss of sigma binding sites in the CA1 area of the anterior hippocampus in Alzheimer's disease correlates with CA1 pyramidal cell loss. Brain Res.
7 Stone J.M., Arstad E., Erlandsson K., Waterhouse R.N., Ell P.J., Pilowsky L.S. (2006). [123I]TPCNE--a novel SPET tracer for the sigma-1 receptor: first human studies and in vivo haloperidol challenge. Synapse.
8 Lever J.R., Gustafson J.L., Xu R., Allmon R.L., Lever S.Z. (2006). Sigma1 and sigma2 receptor binding affinity and selectivity of SA4503 and fluoroethyl SA4503. Synapse.
9 Kawamura K., Ishiwata K., Tajima H., Ishii S., Matsuno K., Homma Y., Senda M. (2000). In vivo evaluation of [(11)C]SA4503 as a PET ligand for mapping CNS sigma(1) receptors. Nucl Med Biol.
10 Waterhouse R.N., Mardon K., Giles K.M., Collier T.L., O'Brien J.C. (1997). Halogenated 4-(phenoxymethyl)piperidines as potential radiolabeled probes for sigma-1 receptors: in vivo evaluation of [123I]-1-(iodopropen-2-yl)-4-[(4-cyanophenoxy)methyl]pip eri dine. J Med Chem.
11 Cobos E.J., Baeyens J.M., Del Pozo E. (2005). Phenytoin differentially modulates the affinity of agonist and antagonist ligands for sigma 1 receptors of guinea pig brain. Synapse.